# Magnetic microbubbles conjugated with anti-vascular cell adhesion molecule-1 monoclonal antibody 429

Chemical name: | Magnetic microbubbles conjugated with anti-vascular cell adhesion molecule-1 monoclonal antibody 429
Abbreviated name: | MBvM
Synonym:
Agent category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Adhesion molecule
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+microbubble)]

Ultrasound is a widely used imaging modality (1), and its role in noninvasive molecular imaging with ligand-carrying microbubbles (MBs) is expanding (2). MBs are comprised of spherical cavities encapsulated in a shell and filled with a gas. The shells are made of phospholipids, surfactants, denatured human serum albumin, or synthetic polymers. Ligands and antibodies can be incorporated into the MB shell surface. MBs are usually 2–8 μm in size. MBs of this size provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (2-4). They also can potentially be used for drug and gene delivery (5).

Endothelial cells are important cells in inflammatory responses (6, 7). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (8).

VCAM-1 is found in very low amounts or nod-detectable on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (9-13). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (14). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. MBs targeted with monoclonal antibody against VCAM-1 are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (15). However, MBs tend to remain close to the axial center of blood vessels and have a small rate of adhesion to the target endothelium (16). Wu et al. (17) prepared magnetic MBs coupled with rat anti-mouse VCAM-1 monoclonal antibody (mAb) 429 (MBvM) to evaluate the efficacy of MBvM to enhance the ultrasound contrast of atherosclerosis in the aorta using a magnetic field guidance system. Their studies showed that the use of MBvM resulted in greater attachment to atherosclerotic aortas in apolipoprotein E (APOE)–deficient mice on a hypercholesterolemic diet (HCD) than did the use of nonmagnetic targeted MBs.

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/gene/7412), APOE (http://www.ncbi.nlm.nih.gov/gene/348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://www.ncbi.nlm.nih.gov/omim/192225), APOE (http://www.ncbi.nlm.nih.gov/omim/107741))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+attachment)]

Wu et al. (17) prepared biotinylated MBs by sonication of an aqueous dispersion of decafluorobutane gas, dipalmitoyl phosphatidylcholine, polyoxyethylene-40-stearate, and distearoylphosphatidylethanolamine-polyethylene glycol(PEG2000)-biotin. MBs were combined with magnetic streptavidin, washed, and conjugated with 0.33 nmol/10^8^ MBs biotinylated rat mAb 429 against mouse VCAM-1 (MBvM) or control inactive mAb (MBiM). Nonmagnetic MBs coupled with mAb 429 (MBv) were prepared similarly using nonmagnetic streptavidin. The three types of MBs were ~2.2 μm in diameter. The streptavidin:mAb:MB ratio was estimated to be ~100,000:300,000:1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+in+vitro)]

Wu et al. (17) performed perfusion of MBvM, MBv, or MBiM (5 × 10^6^/ml) through the flow chamber coated with VCAM-1-Fc chimera at wall shear rates of 1.0–24.0 dynes/cm^2^ (n = 5/group). In the absence of magnetic field guidance, both MBvM and MBv showed ~50 MBs per field at 1 dyne/cm^2^, whereas MBiM showed minimal attachment. The MB attachment decreased with increasing shear rates, with minimal attachment at 8 dynes/cm^2^. In the presence of magnetic field guidance, attachment of MBvM was significantly higher than that of MBv at all shear rates (P < 0.05). There were 260, 120, and 10 MBs at 4 dynes/cm^2^ for MBvM, MBv, and MBiM, respectively. At 20 dynes/cm^2^, there were 80, 0, and 0 MBs for MBvM, MBv, and MBiM, respectively. After termination of magnetic field guidance, MBvM remained firmly attached even at higher shear rates. All experiments were performed in a double-blinded manner.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+rodentia)]

Wu et al. (17) determined MBvM, MBv, or MBiM attachment to excised aorta at 10 min after intravenous injection in wild-type (C57) or APOE-deficient mice on either regular diet (RD) or hypercholesterolemic diet (HCD) (n = 10–14/group). The first 5 min after MB injection was under magnetic field guidance, and then 5 min passed without this guidance. Aortas were removed at 10 min after injection for contrast-enhanced ultrasound (CEU) molecular imaging. Median CEU video intensity signals for MBvM were 28, 15, 9, and 3 for APOE-HCD, APOE-RD, C57-HCD, and C57-RD, respectively. Median CEU video intensity signals for MBv were 10, 6, 3, and 2 for APOE-HCD, APOE-RD, C57-HCD, and C57-RD, respectively. Median CEU video intensity signals for MBiM were 3, 3, 2, and 1 for APOE-HCD, APOE-RD, C57-HCD, and C57-RD, respectively. MBvM provided greater video intensity signals than those of MBv (P < 0.001), which provided greater video intensity signals than MBiM in the four groups of mice (P < 0.001). The aortas from APOE-HCD mice provided the greatest video intensity signals for MBiM compared to the aortas from the other three groups of mice (P < 0.001). Immunohistochemical analysis of the aorta sections showed expression of VCAM-1 in the rank order of APOE-HCD >> APOE-RD > C57-HCD > C57-RD. All experiments were performed in a double-blinded manner. No blocking studies were performed with non-biotinylated mAb 429.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+human)]

No publication is currently available.

## NIH support

R21/33 CA102880

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
5 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
6 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
7 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
8 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
9 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
10 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
11 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
12 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
13 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
14 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
15 Kaufmann B.A., Sanders J.M., Davis C., Xie A., Aldred P., Sarembock I.J., Lindner J.R. (2007). Molecular imaging of inflammation in atherosclerosis with targeted ultrasound detection of vascular cell adhesion molecule-1. Circulation.
16 Lindner J.R., Song J., Jayaweera A.R., Sklenar J., Kaul S. (2002). Microvascular rheology of Definity microbubbles after intra-arterial and intravenous administration. J Am Soc Echocardiogr.
17 Wu J., Leong-Poi H., Bin J., Yang L., Liao Y., Liu Y., Cai J., Xie J. (2011). Efficacy of contrast-enhanced US and magnetic microbubbles targeted to vascular cell adhesion molecule-1 for molecular imaging of atherosclerosis. Radiology.